# ^11^C-Labeled 6-[(3-cyclobutyl-2,3,4,5-tetrahydro-1H-3-benzazepin-7-yl)oxy]-N-methyl-3-pyridinecarboxamide hydrochloride

Chemical name: | ^11^C-Labeled 6-[(3-cyclobutyl-2,3,4,5-tetrahydro-1H-3-benzazepin-7-yl)oxy]-N-methyl-3-pyridinecarboxamide hydrochloride | [image]
Abbreviated name: | [^11^C]GSK189254 | [image]
Synonym: | | [image]
Agent Category: | compound | [image]
Target: | Histamine H_3_ receptor | [image]
Target Category: | Receptor | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^11^C | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Structure of [^11^C]GSK189254.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=h3%20receptor%20review&cmd=DetailsSearch)]

Histamine mediates its activity in the central nervous system (CNS) and the peripheral tissue through four G protein–coupled receptor subtypes (HRs) designated as H_1_, H_2_, H_3_, and H_4_ (1). Among these receptors, the H_3_ subtype that is found primarily in the CNS appears to control several normal physiological processes and is believed to be involved in the development of schizophrenia, epilepsy, attention deficit hyperactive disorder, and Alzheimer’s disease (2). In addition, the H_3_ receptor (H_3_R) is also known to regulate the synthesis and release of histamine itself and other neurotransmitters such as noradrenalin, dopamine, and acetylcholine (1, 2). Several clinical trials (http://clinicaltrials.gov/ct2/results?term=histamine+receptors) approved by the United States Food and Drug Administration (FDA) have either been completed or are in progress to evaluate drugs that modulate HRs for the treatment of diseases involving these receptors. Evidence suggesting the involvement of the H_3_R in a variety of physiological and pathological processes has been obtained only from postmortem studies performed on the human brain, and to confirm these observations investigators believe that it is necessary to perform studies using non-invasive techniques under in vivo conditions.

Several imaging agents have been developed and evaluated for use with non-invasive techniques such as positron emission tomography (PET) and single-photon emission computed tomography to investigate the H_3_R in the brain, but these probes either have a limited uptake in the tissue or show low specificity for or binding to the receptor (2). Recently, two radiolabeled inverse-agonist (3) PET agents with suitable characteristics for the quantification and imaging of the H_3_R have been reported, but these compounds are still under evaluation (4). In a continued effort to develop H_3_R antagonist or reverse-agonist compounds, Medhurst et al. synthesized 6-[(3-cyclobutyl-2,3,4,5-tetrahydro-1H-3-benzazepin-7-yl)oxy]-N-methyl-3-pyridinecarboxamide hydrochloride (GSK189254) and showed that it had a high selectivity for H_3_R under in vitro conditions (5). In addition, the compound was reported to improve the memory and cognitive function of rats with impaired memory and cognition activity, indicating that the drug could be suitable for treating cognitive disorders or dementia in Alzheimer’s disease patients. A GSK189254-duloxetine combination (http://clinicaltrials.gov/ct2/show/related/NCT00387413?term=GSK189254&rank=1) has also been evaluated in a clinical trial for the treatment of electrical hyperalgesia in healthy volunteers; however, no results are as yet available for this study. Because of its in vivo activity and structural characteristics, Plisson et al. labeled GSK189254 with ^11^C ([^11^C]-GSK189254) and evaluated [^11^C]-GSK189254 as a PET imaging agent for H_3_R under in vitro and in vivo conditions in porcine (pig) brain (2). The biodistribution of [^11^C]-GSK189254 in the brain of individuals with mild cognitive impairment has been studied, but, although no publication reporting the results is currently available, the labeled compound appears to be suitable for the quantification of H_3_R in humans, as suggested by Hamill et al. (4).

### Other sources of information regarding histamine H_3_ receptor

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=Fluoroproxyfan18F).

Human H_3_ receptor in OMIM (Online Mendelian Inheritance in Man) (http://www.ncbi.nlm.nih.gov/sites/entrez?db=omim&cmd=DetailsSearch&term=Histamine+H3+receptor&log$=activity).

Human histamine H_3_ receptor Protein (http://www.ncbi.nlm.nih.gov/protein/AAD38151.1?ordinalpos=1&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/AF140538.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) sequences.

Human histamine H_3_ receptor modulating drugs on FDA web site (http://google2.fda.gov/search?q=histamine+H3+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=8).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-GSK189254%20synthesis&cmd=DetailsSearch)]

The synthesis, purification, and identification of [^11^C]-GSK189254 has been detailed by Plisson et al. (2). The radiochemical yield and purity of [^11^C]-GSK189254 was reported to be 80% (based on the incorporation of ^11^C into the radiocompound) and >99% (n = 14), respectively. The specific activity of the labeled compound was reported to be 151 ± 148 GBq/μmol (~4.10 ± 4.0 Ci/μmol) for 14 synthesis reactions at 35 min after the end of bombardment. The purified product was formulated in 0.9% sodium chloride.

Radio-high-performance liquid chromatography (HPLC) analysis of femoral artery plasma obtained from a pig given an injection of [^11^C]-GSK189254 through the femoral vein showed that the intact labeled compound decreased from 88% at 5 min after injection to 55% at 90 min after injection (2). Two metabolites of [^11^C]-GSK189254 were identified with HPLC analysis, and only one was characterized as described by Plisson et al. (2).

In some studies, [^3^H]-R-α-methylhistamine was used (5). This ^3^H-labeled compound was obtained from commercial sources and had a specific activity of 888 GBq/mmol (24 Ci/mmol).

[^3^H]-GSK189254 was also used in some studies (5). This labeled compound was prepared commercially and had a specific activity of 2.99 TBq/mmol (81 Ci/mmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-GSK189254%20in%20vitro%20studies&cmd=DetailsSearch)]

The logD_7.4_ value ofGSK189254 was reported to be 1.74 ± 0.03 (n = 8), as determined with lipophilicity determinations (2).

The incubation of porcine brain with 1 nM [^3^H]-GSK189254 showed that the label was bound primarily in the striatal, cortical, thalamic, hippocampal, hypothalamic, and substantia nigra areas of the brain (2). Very little binding of the label was detected in white matter of the animal brain. Co-incubation of the pig brain slices with excess (10 μM) nonradioactive H_3_R agonists and [^3^H]-GSK189254 was reported to reduce binding of the radiolabel in the striatal area by almost 90%.

Using a [^3^H]-R-α-methylhistamine displacement assay with cell membranes isolated from the brain cortex of several animals, Medhurst et al. reported nonradioactive GSK189254 to have a high affinity for the H_3_R with inhibition constant(pK_i_) values of 9.95 ± 0.15, 8.51 ± 0.11, 8.89 ± 0.13, 8.83 ± 0.09, and 9.61 ± 0.11 for the human, rat, mouse, dog, and pig cortex, respectively (5).

In an in vitro saturation binding study of [^3^H]-GSK189254 with human (n = 1) and rat (n = 4) cortex homogenates, the maximal binding (B_max_) values (receptor density) were determined to be 93.3 and 282.8 ± 8.1 fmol/mg with dissociation constant values of 0.08 and 0.47 ± 0.05 nM, respectively (5). An autoradiographic analysis of the coronal and sagittal section of the rat brain revealed binding of the radiolabel primarily in areas of the brain containing high concentrations of the H_3_R (for details, see Medhurst et al. (5)). Also, incubation of the rat brain slices with [^3^H]-GSK189254 in presence of 10 μM nonradioactive imetit (a strong and highly selective agonist of H_3_R) reduced the binding of the labeled compound to negligible levels in all areas of the brain. With autoradiography, specific binding of [^3^H]-GSK189254 was also observed in the normal human brain cortex, and the labeled compound was shown to bind in the hippocampal CA1 region and the medial temporal cortex in brain sections obtained from patients of Alzheimer’s disease and mild to severe cases of Alzheimer’s disease, respectively (5).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=GSK189254%20rodentia&cmd=DetailsSearch)]

Using [^3^H]-R-α-methylhistamine for ex vivo binding assays with cerebral cortex isolated 2 h postdose from rats (n = 3) previously given increasing oral doses of GSK189254 (0.1–3.0 mg/kg body wt) showed that the estimated mean half maximal effective concentration (ED_50_) for the drug was 0.17 ± 0.03 mg/kg (5). The brain/blood concentration ratio of GSK189254 during the study ranged from 0.9 to 1.2:1, indicating that the drug had good brain penetration. A regression analysis of the brain concentration and receptor occupancy data yielded the brain EC_50_ of GSK189254 to be ~60 nM. For pharmacokinetic properties of GSK189254 in the rat model, see Table 3 in Medhurst et al. (5).

Medhurst et al. (5) showed that acute or repeated doses of GSK189254 were efficacious in several rodent cognition models including passive avoidance, object recognition, and water maze, and the effects were similar to those observed in these models with cholinesterase inhibitors or 5-HT_6_ receptor antagonists. In another study, it was shown that GSK189254 was suitable for the treatment of surgically or virally induced neuropathic pain in rats (6). Using a mouse model, Guo et al. (7) showed that repeat dosing of GSK189254 could be used for the treatment of narcolepsy and daytime sleepiness in the animals.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=GSK189254%20non-primate%20mammals&cmd=DetailsSearch)]

The binding of [^11^C]-GSK189254 in the porcine brain (n = 1–2 animals per study) was studied using PET in anesthetized animals (2). The radioligand was administered as a 1-min bolus to the animals through the femoral vein, and dynamic PET images were acquired immediately and up to 90 min after administration of the tracer. From the images it was evident that the radioligand was easily taken up by the porcine brain, and ~9.0% of the injected dose/L was reported to accumulate in the organ by 20 min after the injection. The distribution of [^11^C]-GSK189254 in the tissue correlated well with the known distribution of H_3_R in the brain of these animals, with the highest accumulation in the striatum, a moderate amount of label in the cortices, and low uptake in the cerebellum. Co-injection of the label with nonradioactive GSK189254 blocked the uptake of the radiocompound, and it was found to be uniformly distributed throughout the porcine brain under these conditions. A dose-dependent blockage of [^11^C]-GSK189254 binding in the brain was reported when the animals were co-treated with the label in the presence of increasing amounts of non-labeled ciproxifan, a known selective antagonist of H_3_R. The in vivo affinity of [^11^C]-GSK189254 for the H_3_R in two animals was reported to be 0.09 and 0.10 nM, respectively, and the estimated B_max_ in different regions of the brain of the two animals were 0.50 and 0.98 nM in the cerebellum, 1.4 and 2.7 nM in the cortex, and 2.1 and 3.2 nM in the striatum.

From these studies, the investigators concluded that [^11^C]-GSK189254 was a suitable PET agent for the imaging of H_3_R in the pig and should be evaluated further for use in humans.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=GSK189254%20non-human%20primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C%20GSK189254%20Human%20Studies&cmd=DetailsSearch)]

The use of [^11^C]-GSK189254 has also been evaluated for the imaging of histamine H_3_ receptors in healthy human subjects (8). Individuals participating in the study (n = 21) were given an intravenous injection of the radiochemical (without, with or after an oral 10 to 100 μg dose of unlabeled GSK189254) and PET scans were obtained over 90 min. Blood samples were taken through the scanning period. The tracer was observed to readily enter the brain and its regional distribution matched the location of the H_3_ receptors i. e. high accumulation in caudate and putamen, medium in the cortical regions, and lowest in the cerebellum. The drug was reported to have a high affinity for theH_3_ receptor and showed a reduced V_T_ at all doses. The oral effective dose resulting in 50% occupation of the receptor was determined to be 4.33 μg.

From these studies the investigators concluded that [^11^C]-GSK189254 was suitable for quantification of the H3 receptors in humans using PET, but a high specific activity tracer is necessary to obtain optimal results (8).

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Garcia-Martin E., Ayuso P., Martinez C., Blanca M., Agundez J.A. (2009). Histamine pharmacogenomics. Pharmacogenomics.
2 Plisson C., Gunn R.N., Cunningham V.J., Bender D., Salinas C.A., Medhurst A.D., Roberts J.C., Laruelle M., Gee A.D. (2009). 11C-GSK189254: a selective radioligand for in vivo central nervous system imaging of histamine H3 receptors by PET. J Nucl Med.
3 Milligan G. (2003). Constitutive activity and inverse agonists of G protein-coupled receptors: a current perspective. Mol Pharmacol.
4 Hamill T.G., Sato N., Jitsuoka M., Tokita S., Sanabria S., Eng W., Ryan C., Krause S., Takenaga N., Patel S., Zeng Z., Williams D., Sur C., Hargreaves R., Burns H.D. (2009). Inverse agonist histamine H3 receptor PET tracers labelled with carbon-11 or fluorine-18. Synapse.
5 Medhurst A.D., Atkins A.R., Beresford I.J., Brackenborough K., Briggs M.A., Calver A.R., Cilia J., Cluderay J.E., Crook B., Davis J.B., Davis R.K., Davis R.P., Dawson L.A., Foley A.G., Gartlon J., Gonzalez M.I., Heslop T., Hirst W.D., Jennings C., Jones D.N., Lacroix L.P., Martyn A., Ociepka S., Ray A., Regan C.M., Roberts J.C., Schogger J., Southam E., Stean T.O., Trail B.K., Upton N., Wadsworth G., Wald J.A., White T., Witherington J., Woolley M.L., Worby A., Wilson D.M. (2007). GSK189254, a novel H3 receptor antagonist that binds to histamine H3 receptors in Alzheimer's disease brain and improves cognitive performance in preclinical models. J Pharmacol Exp Ther.
6 Medhurst S.J., Collins S.D., Billinton A., Bingham S., Dalziel R.G., Brass A., Roberts J.C., Medhurst A.D., Chessell I.P. (2008). Novel histamine H3 receptor antagonists GSK189254 and GSK334429 are efficacious in surgically-induced and virally-induced rat models of neuropathic pain. Pain.
7 Guo R.X., Anaclet C., Roberts J.C., Parmentier R., Zhang M., Guidon G., Buda C., Sastre J.P., Feng J.Q., Franco P., Brown S.H., Upton N., Medhurst A.D., Lin J.S. (2009). Differential effects of acute and repeat dosing with the H3 antagonist GSK189254 on the sleep-wake cycle and narcoleptic episodes in Ox-/- mice. Br J Pharmacol.
8 Ashworth S., Rabiner E.A., Gunn R.N., Plisson C., Wilson A.A., Comley R.A., Lai R.Y., Gee A.D., Laruelle M., Cunningham V.J. (2010). Evaluation of 11C-GSK189254 as a novel radioligand for the H3 receptor in humans using PET. J Nucl Med.